# [[5'-(4-Hydroxyphenyl)[2,2’-bithiophen]-5-yl]methylene]-propanedinitrile NIAD-4

Chemical name: | [[5’-(4-Hydroxyphenyl)[2,2’-bithiophen]-5-yl]methylene]-propanedinitrile
Abbreviated name: | NIAD-4
Synonym:
Backbone: | Compound
Target: | Amyloid-β (Aβ)
Mechanism: | Specific binding
Method of detection: | Optical, red fluorescence imaging
Source of signal: | NIAD-4
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28amyloid-beta%20binding%20fluorophore%29%20OR%20%28amyloid%20optical%20imaging%29)]

[[5’-(4-Hydroxyphenyl)[2,2’-bithiophen]-5-yl]methylene]-propanedinitrile (NIAD-4) is a fluorophore that was developed for optical imaging of amyloid-β (Aβ) in the central nervous system (CNS) in basic and pre-clinical research for Alzheimer’s disease (AD).

Aβ-peptide was sequenced from the meningeal blood vessels of AD patients and individuals with Downs syndrome (1). Aβ peptides contain 40-42 amino acid residues and are metabolic products of Aβ precursor protein (APP) from cleavage by β− and γ−secretases . Aβ is also identified as the primary component of the neuritic plaques of AD patient brain tissue (2). The cloning of the gene encoding the APP and its localization to chromosome 21 led to the hypothesis that Aβ accumulation is the primary event in AD pathogenesis (1, 3). This hypothesis proposes that neuronal death in AD is related to toxic effect of Aβ on the adjacent cell bodies or cell processes (4). AD is a progressive, neurogenerative disorder of the CNS, and is characterized by a common set of clinical and pathological features . In addition to Aβ, the microtubule-associated protein, tau (זּ), is also found in the cell body and axons of neurons as neurofibrillary tangles.

The search for a cure or effective treatment of AD requires in vivo detection and quantification of Aβ in the brain for evaluation of the efficacy of AD therapy . Various amyloid-imaging probes have been developed based on positron emission tomography, single-photon emission computed tomography, and optical imaging. Optical imaging is an imaging method that utilizes light photons emitted from bioluminescence and fluorescence probes (5). Fluorescence imaging in the visible light range of 395-600 nm can penetrate only to a depth of 1−2 cm and has significant background signal because of tissue autofluorescence. Depth penetration is one major limiting factor in in vivo optical imaging. Currently, in vivo optical imaging has wide applications in small animal imaging but only limited applications in large animal and human studies (6). Near-Infrared (NIR) (light range 650−900 nm) fluorescence imaging has the advantages of relatively higher tissue penetration and lower autofluorescence from nontarget tissue. One promising approach of developing optical imaging probes is based on the development of small-molecules of Aβ−staining compounds, such as Congo red and thioflavin T. The specific binding of these compounds to Aβ aggregates is believed to be a combination of electrostatic interactions of the compounds with the Aβ protein, and the compound’s shape is complementary to Aβ’s surface whichinvolves hydrophobic interactions with the planarized aromatic Л system of the compound (7, 8). In an effort to produce an in vivo optical imaging probe which gives specific far-red fluorescence, Nesterov et al. (7) developed NIAD-4 which has a relatively low molecular weight of 334 Da and a dithienyl-ethenyll Л-conjugated bridge between donor and acceptor. NIAD-4 has a structure geometry that is readily planarized and results in a red shift upon binding to Aβ. The highly polarizable bridge provides a substantial bathochromic shift in both absorption and emission spectra of the agent. The rigid rodlike aromatic core of the agent is designed to achieve high specific binding to Aβ aggregrates. NIAD-4 is commercially (http://www.nomadics.com/lifesciences) available for in vitro/in situ applications and in vivo imaging in animal research.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28amyloid-beta%20binding%20fluorophore%29%20OR%20%28amyloid%20optical%20imaging%29%29%20AND%20synthesis)]

Nesterov et al. (7) reported the preparation of NIAD-4 in a three-step synthesis based on Stille coupling. Briefly, 4-iodo-1-tert-butyl-dimethylsiloxylbenzene was reacted with 5-tributylstannyl-2,2’-bithiophene at 70ºC for 36 h with a yield of 57%. The resulting product was converted to the silyl-protected aldehyde using N,N,N’,N’-tetramethylethylenediamine and malononitrile with a yield of 84%. The final step involved in situ deprotection using hydrochloric acid at 60ºC for 6 h with a yield of 77%. The chemical purity of the final product was >95%. The final product was a dark-red material that exhibited a bright red fluorescence (625 nm) in methanol solution (quantum yield = 15%). NIAD-4 stored in the dark at −20ºC was stable for 6 months.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28amyloid-beta%20binding%20fluorophore%29%20OR%20%28amyloid%20optical%20imaging%29%29%20AND%20in%20vitro)]

Nesterov et al. (7) characterized the properties of NIAD-4 in vitro. The agent was only slightly soluble in aqueous media. At concentrations above ≈10 μM, NIAD-4 formed micelles/aggregates. The aqueous solutions of NIAD-4 only had trace fluorescent emission of quantum yield ≈ 0.008%. In the presence of aggregated Aβ protein (≈ 10 μM), there was a dramatic enhancement of the fluorescent emission with a quantum yield of 5% (NIAD-4 = 4.1 μM in phosphate-buffered saline). There was also a significant red shift (Δג ≈ 70 nm) and a 1.3-fold increase in the extinction coefficient. In vitro binding studies with artificially aggregated Aβ protein indicated that NIAD-4 bound to the same Aβ sites as BTA-1 (9), a known high-affinity Aβ-binding compound. The studies showed that NIAD-4 had a binding affinity (K_i_) of 10 nM. In comparison, thioflavin T had K_i_ of 580 nM.

Nesterov et al. (7) studied the specificity of NIAD-4 binding to Aβ by In situ histochemical staining of fixed sections from transgenic mouse brain. Brain sections were obtained from aged APP transgenic mice with AD-like pathology. The brain sections were labeled with a NIAD-4 (10 μM) solution in DMSO/propylene glycol for 15 min at room temperature. In vitro fluorescence imaging showed high-specificity labeling of NIAD-4 which revealed the exact position and size of the aggregated Aβ deposits.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28amyloid-beta%20binding%20fluorophore%29%20OR%20%28amyloid%20optical%20imaging%29%29%20AND%20rodentia)]

Nesterov et al. (7) demonstrated the in vivo Aβ binding of NIAD-4 in aged APP transgenic mice. Mice were prepared with cranial windows to allow direct monitoring of the brain surface and then administered 10 μM of 2 mg/kg NIAD-4 solution by i.v. injection. Red fluorescence imaging using multiphoton microscopy showed that the agent readily crossed the blood-brain barrier and labeled specifically both the plaques and cerebrovascular amyloid angiopathy.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28amyloid-beta%20binding%20fluorophore%29%20OR%20%28amyloid%20optical%20imaging%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28amyloid-beta%20binding%20fluorophore%29%20OR%20%28amyloid%20optical%20imaging%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28amyloid-beta%20binding%20fluorophore%29%20OR%20%28amyloid%20optical%20imaging%29%29%20AND%20human)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

NIAD4 for Alzheimer’s Disease Poster 1.

NIAD4 for Alzheimer’s Disease Poster 2

## NIH Support

NIH grant EB00768.

## References

1 Hardy J., Selkoe D.J. (2002). The amyloid hypothesis of Alzheimer's disease: progress and problems on the road to therapeutics. Science.
2 Masters C.L., Multhaup G., Simms G., Pottgiesser J., Martins R.N., Beyreuther K. (1985). Neuronal origin of a cerebral amyloid: neurofibrillary tangles of Alzheimer's disease contain the same protein as the amyloid of plaque cores and blood vessels. Embo J.
3 Kang J., Lemaire H.G., Unterbeck A., Salbaum J.M., Masters C.L., Grzeschik K.H., Multhaup G., Beyreuther K., Muller-Hill B. (1987). The precursor of Alzheimer's disease amyloid A4 protein resembles a cell-surface receptor. Nature.
4 Carter J., Lippa C.F. (2001). Beta-amyloid, neuronal death and Alzheimer's disease. Curr Mol Med.
5 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
6 Bremer C., Ntziachristos V., Weissleder R. (2003). Optical-based molecular imaging: contrast agents and potential medical applications. Eur Radiol.
7 Nesterov E.E., Skoch J., Hyman B.T., Klunk W.E., Bacskai B.J., Swager T.M. (2005). In vivo optical imaging of amyloid aggregates in brain: design of fluorescent markers. Angew Chem Int Ed Engl.
8 Khurana R., Uversky V.N., Nielsen L., Fink A.L. (2001). Is Congo red an amyloid-specific dye?. J Biol Chem.
9 Klunk W.E., Wang Y., Huang G.F., Debnath M.L., Holt D.P., Shao L., Hamilton R.L., Ikonomovic M.D., DeKosky S.T., Mathis C.A. (2003). The binding of 2-(4'-methylaminophenyl)benzothiazole to postmortem brain homogenates is dominated by the amyloid component. J Neurosci.